# 4-[^18^F]Fluoro-L-m-tyrosine

Chemical name: | 4-[^18^F]Fluoro-L-m-tyrosine
Abbreviated name: | 4-[^18^F]FMT
Synonym: | 4-FMT, 4-[^18^F]Fluoro-3-hydroxy-L-phenylalanine
Agent Category: | Compound
Target: | Aromatic L−amino acid decarboxylase (AAAD)
Target Category: | Enzyme-substrate
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-FMT%20OR%2018F%204-FMT%20OR%204-fluoro-L-m-tyrosine)]

4-[^18^F]Fluoro-L-m-tyrosine (4-[^18^F]FMT) is a noncatecholic radioligand developed for positron emission tomography (PET) imaging of dopaminergic metabolism and function in the central nervous system (CNS) (1, 2). It is an analog of dihydroxyphenylalanine (L-DOPA) labeled with ^18^F, a positron emitter with a physical t_½_ of 109.7 min.

Dopamine is an important neurotransmitter that regulates and controls human movement, motivation, and cognition (3). It is also associated with human behaviors such as reward, reinforcement, and addiction. There are four main dopaminergic pathways in the CNS (4). Two pathways that originate in the ventral tegmental area project toward the cortex and the limbic area, a third pathway projects from the hypothalamus toward the pituitary gland, and a fourth pathway projects from the substantia nigra to the striatum. Neurons located in these pathways release dopamine as a neurotransmitter at their terminals. There are five known dopamine receptor subtypes, which are categorized as D_1_-like or D_2_-like (5). The D_1_-like receptor subtypes (D_1_ and D_5_) couple with the Gs protein to activate adenylyl cyclase, and the D_2_-like subtypes (D_2_, D_3_, and D_4_) couple with G proteins to inhibit adenylate cyclase. Abnormal changes in the dopaminergic system can lead to pathologic conditions such as Parkinson’s disease, schizophrenia, Huntington’s disease, depression, Gilles de la Tourette syndrome, narcolepsy and other neuropsychiatric disorders (6).

Radiotracer imaging with specific radiolabeled molecular probes can measure pre-, post-, and intrasynaptic aspects of the dopaminergic system (6). [^18^F]Fluoro-L-dopa ([^18^F]FDOPA), which was developed by Firnau et al. (7), was the first presynaptic probe to be developed. It was also the first molecular probe used by Garnett et al. (8) to visualize human brain dopamine in vivo. Like endogenous L-DOPA, [^18^F]FDOPA is converted by the enzyme aromatic L-amino acid decarboxylase (AAAD) to the dopamine analog fluorodopamine. Thus, PET imaging of [^18^F]FDOPA allows in vivo visualization and assessment of dopamine function in the brain. However, the use of [^18^F]FDOPA is complicated by the peripheral metabolism of this agent. DeJesus et al. (9) proposed the synthesis and use of [^18^F]FMT and other tyrosine analogs as possible alternative dopamine probes because they lack the enediol moiety required of catecholamine-O-methyltransferase (COMT) substrates. Both o- and m-tyrosines are excellent substrates for AAAD but m-tyrosine is a normal constituent in the brain (10). Three isomers of [^18^F]FMT, 2-, 4-, and 6-[^18^F]FMT, were initially produced and studied (11) Both 4-[^18^F]FMT and 6-[^18^F]FMT appeared promising as early studies showed that they provided good image contrast (1, 12, 13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%284-FMT%20OR%2018F%204-FMT%20OR%204-fluoro-L-m-tyrosine%29%20AND%20synthesis)]

DeJesus et al. (9, 11) reported the synthesis of [^18^F]FMT via direct electrophilic fluorination of D,L-m-tyrosine with acetyl[^18^F]hypofluorite ([^18^F]AcOF). [^18^F]F_2_ was produced from [^18^O]O_2_ by a two-bombardment method. The final labeled product was purified by high-performance liquid chromatography (HPLC). HPLC analysis showed that approximately 80% of the D,L-m-tyrosine had reacted, and ^19^F-NMR analysis indicated that the final product was a mixture of 2-, 4-, and 6-[^18^F]FMT isomers in the proportion of ≈36:11:52, respectively. The radiochemical yield was 71 ± 5% (n = 3; decay correction based on [^18^F]AcOF activity) after purification. The specific activity was 3.7−7.4 GBq/mmol (100−200 mCi)/mmol).

Perlumtter et al. (14) prepared 4-[^18^F]FMT by using regioselective fluorodemercuration of a 4-mercurio precursor with ^18^F-labeled acetylhypofluorite. The mucurio precursor was synthesized in a three-step sequence from 3-hydroxy-L-phenylalanine. 3-hydroxy-L-phenylalanine ethyl ester was obtained by refluxing 3-hydroxy-L-phenylalanine in absolute ethanol saturated with dry hydrogen chloride for 5 h. This ethyl ester compound was reacted with di-t-butyl dicarbonate at room temperature under argon for 24 h to give N-(t-butoxycarbonyl)-3-hydroxy-L-phenylalanine ethyl ester. The resulting compound was then reacted with mercuric trifluoroacetate at room temperature for 5 days. The bulky t-butoxycarbonyl N-protecting group facilitated the specific precipitation of the mercurio precursor from the reaction mixture. Radiosynthesis was carried out by bubbling ^18^F-labeled acetylhypofluorite into a solution of the mercurio precursor at room temperature for 10 min. The solvent was evaporated, and the residue was hydrolyzed with 55% hydrogen iodide. The radiochemical yield was 25% (corrected for decay) with a synthesis time of ~60 min. The chemical, radiochemical, and enantiomeric purities were >99%, and the specific activity was ~74 GBq/mmol (2 Ci/mmol) at the end of the synthesis.

Namavari et al. (15) described the synthesis of 4-[^18^F]FMT based on a regioselective radiofluorodestannylation procedure. In this method, N-(trifluoroacetyl)-3-acetoxy-4-(trimethylstannyl)-L-phenylalanine ethyl ester was first synthesized as a precursor. The radiosynthesis was carried out by electrophilic fluorodestannylation of the precursor and exhaustive deprotection of the acid, amine, and phenol. Briefly, ^18^F-labeled fluorine was bubbled into a solution of the trimethyltin derivative in Freon-11 at room temperature for 15 min. After purification by chromatography, the radiolabeled intermediate was hydrolyzed with 48% hydrogen bromide at 130ºC for 10 min. The reaction mixture was partially neutralized with 3-N sodium hydroxide and then purified by HPLC. More than 99% of the 4-[^18^F]FMT was chemically and radiochemically pure. Chiral HPLC determined the enantiomeric purity to be >99% and the total tin determined by inductively coupled plasma spectrometry was <15 parts per billion. The total synthesis time was 60 min, and the radiochemical yield was 11% at the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-FMT%20OR%2018F%204-FMT%20OR%204-fluoro-L-m-tyrosine%29%20AND%20in%20vitro)]

DeJesus et al. (2) used rat striatal synaptosomes to evaluate whether 4-[^18^F]FMT was a good dopa decarboxylase substrate. For 4-[^18^F]FMT, the Michaelis constant (K_m_) was determined to be 54 μM and V_max_ was 450 pmol/min per g. In comparison, 6-[^18^F]FMT had K_m_ = 53 μM and V_max_ = 390 pmol/min per g.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%284-FMT%20OR%2018F%204-FMT%20OR%204-fluoro-L-m-tyrosine%29%20AND%20rodentia)]

Melega et al. (1) conducted central and peripheral metabolism studies of 4-[^18^F]FMT in rats. 4-[^18^F]FMT was injected as an i.v. dose of 51.8 MBq/kg (1.4 mCi/kg) in rats pretreated with 5 mg/kg s.c. carbidopa, an AAAD inhibitor. Specific brain radioactivity localization (striatum/cerebellum ratio = 1.7 n = 4) was observed at 30 min. HPLC analysis showed that 66 ± 5% of the striatal radioactivity was associated with 4-fluoro-3-hydroxyphenylacetic acid (FPAC), 19 ± 3% was 4-fluoro-3-hydroxyphenylethylamine (FMA), 5 ± 1% was O-sulfoconjugate (FMA-sulfate), and only 9 ± 4% was 4-[^18^F]FMT. The formation of FPAC was mediated by central monoamine oxidase (MAO) oxidation, and the formation of FMA was mediated by AAAD decarboxylation. In the plasma, 67 ± 11% of the radioactivity at 30 min was 4-[^18^F]FMT , 27 ± 7% was FMA sulfate, and 7± 2% was FPAC. The plasma level of 4-[^18^F]FMT was 60% at 120 min.

In direct comparisons between 4-[^18^F]FMT, 6-[^18^F]FMT and [^18^F]FDOPA, Barrio et al. (12) conducted regional brain distribution and peripheral metabolism studies of these radioligands in rats. Each rat received 51.8 MBq/kg (1.4 mCi/kg) of radioactivity by i.v. administration and carbidopa s.c. 60 min before the radioligand injection. The distribution of striatal metabolites of 4-[^18^F]FMT appeared to be different from that of FDOPA or 6-[^18^F]FMT. At 30 min after injection, 66 ± 5% of the 4-[^18^F]FMT radioactivity had converted to 4-FPAC whereas the predominant metabolite of 6-[^18^F]FMT and [^18^F]FDOPA was 6-FMA. In peripheral metabolism, both 4-[^18^F]FMT and 6-[^18^F]FMT produced measurable amounts of decarboxylation metabolites even with carbidopa pretreatment. The authors related this finding to the AAAD activity that is higher in rat serum (60.0 pmol/min per ml) than in human serum (≈1 pmol/mn per ml) (16).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%284-FMT%20OR%2018F%204-FMT%20OR%204-fluoro-L-m-tyrosine%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%284-FMT%20OR%2018F%204-FMT%20OR%204-fluoro-L-m-tyrosine%29%20AND%20%28primate%20NOT%20human%29)]

PET studies of 4-[^18^F]FMT were conducted in monkeys (n = 3) with doses of 185-370 MBq (5−10 mCi) and specific activity of 37−74 GBq/mmol (1−2 Ci/mmol) (1). Three monkeys were pretreated with 5 mg/kg i.v. carbidopa 60 min before 4-[^18^F]FMT injection. PET imaging showed rapid radioactivity accumulation in striatal structures and rapid clearance from the cerebellum. The striatum/cerebellum radioactivity ratio increased to ≈4 at 3 h. Little radioactivity was observed in the bone structures. Chemical analysis of arterial plasma showed that 4-[^18^F]FMT remained the predominant species and decreased to 60% of the total radioactivity at 120 min. FMA-sulfate slowly increased to ≈35% at 120 min and FPAC remained at <6%.

Barrio et al. (12) studied the in vivo kinetic and biochemical behaviors of 4-[^18^F]FMT in three monkeys. Each monkey received ≈37 MBq/kg (1 mCi/kg) i.v. 4-[^18^F]FMT after 1 h pretreatment with 5 mg/kg carbidopa. PET imaging at 90−120 min after injection showed that the radioactivity accumulation pattern was consistent with localization of central dopamine-rich structures, but also showed accumulated in AAAD-rich innervation sites. The striatum/cerebellum ratios were 2.76 ± 0.20, 3.48 ± 0.40, and 4.57 ± 1.16 at 60 min, 90 min, and 120 min, respectively. In comparison, [^18^F]FDOPA had ratios of 1.47 ± 0.15, 1.85 ± 0.17, and 2.06 ± 0.09, respectively. Peripherally, no COMT-mediated products were produced, but products of AAAD-mediated decarboxylation were found. The AAAD activity in monkey serum was 44.7 pmol/min per ml (16). The AAAD-mediated decarboxylation produced 4-FMA which was then converted to FPAC by MAO oxidation or conjugated by phenolsulfotransferase. In comparison, 6-FMA produced from 6-[^18^F]FMT was not subject to the same peripheral MAO oxidation.

Hayase et al. (17) reported that PET imaging of 4-[^18^F]FMT in monkeys showed specific accumulation in AAAD-rich areas of the striatum, which reached a striatum/cerebellum ratio of 3 at 2 h. In a study with four monkeys rendered hemi-Parkinsonian by unilateral intracarotid artery infusion of the neurotoxin 1-methyl-4-phenyl-1,2,3,6-tetrahydropyridine (MPTP), Hayase et al. (18) used 4-[^18^F]FMT imaging to show a reduction in AAAD activity in the MPTP-lesioned striatum. The mean lesioned-striatum/cerebellum ratio was 1.3 compared with 3.9 in the normal contralateral region.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=4-FMT%20OR%2018F%204-FMT%20OR%204-fluoro-L-m-tyrosine%29%20AND%20human)]

No publication is currently available.

## References

1 Melega WP, Perlmutter MM, Luxen A, Nissenson CH, Grafton ST, Huang SC, Phelps ME, Barrio JR. (1989). 4-[18F]fluoro-L-m-tyrosine: an L-3,4-dihydroxyphenylalanine analog for probing presynaptic dopaminergic function with positron emission tomography. J Neurochem.
2 DeJesus OT, Murali D, Nickles RJ. (1995). Synthesis of brominated and fluorinated ortho-tyrosine analogs as potential DOPA decarboxylase tracers. J Label. Comp. Radiopharm.
3 Volkow ND, Fowler JS, Gatley SJ, Logan J, Wang GJ, Ding YS, Dewey S. (1996). PET evaluation of the dopamine system of the human brain. J Nucl Med.
4 Dailly E, Chenu F, Renard CE, Bourin M. (2004). Dopamine, depression and antidepressants. Fundam Clin Pharmacol.
5 5. Wagner HNJ, Szabo Z. Research and clinical applications of neuroreceptor imaging, in Handbook of Radiopharmaceuticals, M.J. Welch and C.S. Redvanly, Editors. 2003, John Wiley & Sons, Ltd: West Sussex, . p. 582-602.
6 Verhoeff NP. (1999). Radiotracer imaging of dopaminergic transmission in neuropsychiatric disorders. Psychopharmacology (Berl).
7 Firnau G, Nahmias C, Garnett S. (1973). The preparation of (18 F)5-fluoro-DOPA with reactor-produced fluorine-18. Int J Appl Radiat Isot.
8 Garnett ES, Firnau G, Nahmias C. (1983). Dopamine visualized in the basal ganglia of living man. Nature.
9 DeJesus OT, Mukherjee J, Appelman EH. (1989). Synthesis of O- and M-thyrosine analogs as potential tracers for CNS dopamine. J Label Comp Radiopharm.
10 Boulton AA. (1976). Identification, distribution, metabolism, and function of meta and para tyramine, phenylethylamine and tryptamine in brain. Adv Biochem Psychopharmacol.
11 DeJesus OT, Sunderland JJ, Nickles JR, Mukherjee J, Appelman EH. (1990). Synthesis of radiofluorinated analogs of m-tyrosine as potential L-dopa tracers via direct reaction with acetylhypofluorite. Int J Rad Appl Instrum [A].
12 Barrio JR, Huang SC, Yu DC, Melega WP, Quintana J, Cherry SR, Jacobson A, Namavari M, Satyamurthy N, Phelps ME. (1996). Radiofluorinated L-m-tyrosines: new in-vivo probes for central dopamine biochemistry. J Cereb Blood Flow Metab.
13 DeJesus OT, Endres CJ, Shelton SE, Nickles RJ, Holden JE. (1997). Evaluation of fluorinated m-tyrosine analogs as PET imaging agents of dopamine nerve terminals: comparison with 6-fluoroDOPA. J Nucl Med.
14 Perlmutter M, Satyamurthy N, Luxen A, Phelps ME, Barrio JR. (1990). Synthesis of 4-[18F]fluoro-L-m-tyrosine: a model analog for the in vivo assessment of central dopaminergic function. Int J Rad Appl Instrum [A].
15 Namavari M, Satyamurthy N, Phelps ME, Barrio JR. (1993). Synthesis of 6-[18F] and 4-[18F]fluoro-L-m-tyrosines via regioselective radiofluorodestannylation. Appl Radiat Isot.
16 Rahman MK, Nagatsu T, Kato T. (1981). Determination of aromatic L-amino acid decarboxylase in serum of various animals by high-performance liquid chromatography with electrochemical detection. Life Sci.
17 Hayase N, Tomiyoshi K, Watanabe K, Horikoshi S, Hirato M, Shibasaki T, Ohye C. (1994). Visualization of dopamine nerve terminals in monkey by positron emission tomography using 4-[18F]fluoro-L-m-tyrosine. Stereotact Funct Neurosurg.
18 Hayase N, Tomiyoshi K, Watanabe K, Horikoshi S, Shibasaki T, Ohye C. (1995). Positron emission tomography with 4-[18F]fluoro-L-m-tyrosine in MPTP-induced hemiparkinsonian monkeys. Ann Nucl Med.